# VivoTag-S 680-anti-human mammaglobin-A monoclonal antibody

Chemical name: | VivoTag-S 680-anti-human mammaglobin-A monoclonal antibody
Abbreviated name: | MamAb-680
Synonym:
Agent category: | Antibody
Target: | Mammaglobin-A (SCGB2A2)
Target category: | Antigen
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | VivoTag 680 (VT680)
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MamAb-680)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive compliment to radionuclide imaging in small animals.

The primary function of the lymphatic system is to drain ~10% of the interstitial fluid from small capillaries to lymphatic vessels through lymph nodes (LNs) and finally to the venous system (4-8). LNs form a natural filter for the lymphatic drainage and prevent the possible migration of cancer cells from the lymphatic system into the rest of the body or into the venous system. As the first LN that receives lymph drainage from a tumor bed, the sentinel LN is very likely to contain cancer cells if the primary tumor has spread via the lymphatic system. However, with advances of new imaging agents and techniques, imaging and mapping of both the lymphatic vessels and the LNs are now possible with x-ray–computed tomography, ultrasound, nuclear medicine, and magnetic resonance imaging (9-11). If the sentinel LN contains tumor cells, then the axillary LNs (ALNs) will be evaluated further for the presence of tumor cells. Therefore, there is a need for a specific biomarker for identification of ALNs containing tumor cells.

Mammaglobin-A belongs to a family of epithelial secretory proteins (secretoglobins). Mammaglobin-A gene (SCGB2A2) encodes a 10.5-kDa glycoprotein that is exclusively expressed in normal breast tissue. In an analysis of 35 breast tumor biopsies, mammaglobin-A mRNA levels increased at least ten-fold relative to normal breast tissue in 23% of cases (12). In another study, mammaglobin-A protein levels increased drastically in 81 of 100 breast tumors (13). Mammaglobin-A can be used as a biomarker for the detection of breast tumor micrometastasis in sentinel LNs (14). Tafreshi et al. (15) performed mammaglobin-A protein expression studies in 250 breast cancer samples showing positive staining in ~90% of invasive ductal carcinoma, 80% of intraductal carcinoma, and 45% of LN with macrometastasis. Tafreshi et al. (15) conjugated the NIR fluoresecent dye VivoTag-S 680 to a murine monoclonal antibody against human mammaglobin-A (MamAb) as an imaging probe (MamAb-680) for the noninvasive detection of breast tumor metastasis in LNs in mice.

### Related Resource Links:

- Chapters in MICAD (Mammaglobin-A (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Mammaglobin-A+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Mammaglobin-A (http://www.ncbi.nlm.nih.gov/gene/4250))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Mammaglobin-A (http://www.ncbi.nlm.nih.gov/omim/605562))
- Clinical trials (Mammaglobin-A (http://www.clinicaltrials.gov/ct2/results?term=mammaglobin-A))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MamAb-680%20and%20synthesis)]

Tafreshi et al. (15) prepared MamAb-680 by incubation of 0.1 nmol MamAb with 0.01 mg VivoTag-S 680. MamAb-680 was purified with column chromatography. VivoTag-S 680 exhibits an excitation peak at 673 nm and an emission peak at 691. The number of dye molecules per antibody was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MamAb-680%20and%20in%20vitro)]

Human ZR-75.1 breast cancer cells express high levels of mRNA for mammaglobin-A, whereas human MDA-MB-231 breast cancer cells express no detectable level (15). Confocal microscopy analysis showed that MamAb-680 bound to the cell surface of ZR-75.1 cells but did not bind to MDA-MB-231 cell surface. No immunoreactivity or sites per cell were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MamAb-680%20and%20rodentia)]

Tafreshi et al. (15) performed a series of whole-body NIR fluorescence imaging studies in nude mice (n = 4) bearing a ZR-75.1 tumor in the right mammary fat pad (MFP) and an MDA-MB-231 tumor in the left MFP at 24 h after intravenous injection of 0.33 nmol MamAb-680. There was an 8.6 ± 0.8-fold enhancement observed in the positive tumor compared to the negative tumor. Preinjection of MamAb (1.65 nmol) reduced the enhancement by 6.6-fold in the positive tumor. Ex vivo biodistribution showed that the positive tumor had the highest signal intensity at 24 h after injection, whereas the negative tumor and the normal tissues showed <15% of the positive tumor signal intensity at the same time point. The signal intensity of ZR-75.1 tumor peaked at ~24 h and gradually declined to background level by 12 days after injection.

In another experiment, MamAb-680 was injected into the MFP of mice bearing ALN metastases of ZR-75.1 tumor cells. At 24 h, a strong NIR fluorescence signal was detected in the area of the ALNs, which contained ZR-75.1 tumor cells as confirmed with immunohistostaining and pathological examination ex vivo. At least 1,000 ZR-75.1 tumor cells were detectable above background. MamAb-680 was able to travel through the lymphatic system from the MFP to the ALNs. A clear signal in the ALNs was still detected up to 7 days after injection of MamAb-680. No signal was obtained in the tumor-negative ALNs.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MamAb-680%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MamAb-680%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MamAb-680%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Clement O., Luciani A. (2004). Imaging the lymphatic system: possibilities and clinical applications. Eur Radiol.
5 Styblo T., Aarsvold J.N., Grant S.F., Cohen C., Larsen T., Waldrop S., Alazraki N.P. (2001). Sentinel lymph nodes: optimizing success. Semin Roentgenol.
6 Hoh C.K., Wallace A.M., Vera D.R. (2003). Preclinical studies of [(99m)Tc]DTPA-mannosyl-dextran. Nucl Med Biol.
7 Salem C.E., Hoh C.K., Wallace A.M., Vera D.R. (2006). A preclinical study of prostate sentinel lymph node mapping with [99mTC]diethylenetetramine pentaacetic acid-mannosyl-dextran. J Urol.
8 Vera D.R., Wallace A.M., Hoh C.K., Mattrey R.F. (2001). A synthetic macromolecule for sentinel node detection: (99m)Tc-DTPA-mannosyl-dextran. J Nucl Med.
9 Luciani A., Itti E., Rahmouni A., Meignan M., Clement O. (2006). Lymph node imaging: basic principles. Eur J Radiol.
10 Wunderbaldinger P. (2006). Problems and prospects of modern lymph node imaging. Eur J Radiol.
11 Schoder H., Glass E.C., Pecking A.P., Harness J.K., Wallace A.M., Hirnle P., Alberini J.L., Vilain D., Larson S.M., Hoh C.K., Vera D.R. (2006). Molecular targeting of the lymphovascular system for imaging and therapy. Cancer Metastasis Rev.
12 Watson M.A., Fleming T.P. (1996). Mammaglobin, a mammary-specific member of the uteroglobin gene family, is overexpressed in human breast cancer. Cancer Res.
13 Watson M.A., Dintzis S., Darrow C.M., Voss L.E., DiPersio J., Jensen R., Fleming T.P. (1999). Mammaglobin expression in primary, metastatic, and occult breast cancer. Cancer Res.
14 Zehentner B.K., Carter D. (2004). Mammaglobin: a candidate diagnostic marker for breast cancer. Clin Biochem.
15 Tafreshi N.K., Enkemann S.A., Bui M.M., Lloyd M.C., Abrahams D., Huynh A.S., Kim J., Grobmyer S.R., Carter W.B., Vagner J., Gillies R.J., Morse D.L. (2011). A mammaglobin-A targeting agent for noninvasive detection of breast cancer metastasis in lymph nodes. Cancer Res.